# Gadoxetate

Chemical name: | Gadoxetate
Abbreviated name: | Gd-EOB-DTPA
Synonym: | Eovist^®^, Primovist™, gadoxetic acid, gadolinium-ethoxybenzyl-diethylenetriaminepentaacetic acid, disodium S-[4-(4-ethoxybenzyl)-3,6,9-tris[(carboxy-_K_O)methyl]-3,6,9-triazaundecandioato) (5-)-_K_^3^N^3^,N^6^,N^9^,_K_^2^O^1^,O^11^]gadolinite (2-), gadolinium ethoxybenzyl-DTPA, gadoxate disodium
Agent Category: | Compound
Target: | Hepatocyte, liver, biliary tract
Target Category: | Uptake by the hepatocytes
Method of detection: | Magnetic resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium)]

Gadoxetate (Gd-EOB-DTPA) is a paramagnetic contrast agent developed for tissue contrast enhancement in hepatobiliary magnetic resonance imaging (MRI) (1-3).

Conventional paramagnetic contrast agents are generally metal chelates with unpaired electrons, and they work by shortening both the t_1_ and t_2_ relaxation times of surrounding water protons to produce a signal-enhancing effect (4, 5). At normal clinical doses of 0.1−0.2 mmol/kg, the t_1_ effect tends to dominate. Current agents are water-soluble compounds that distribute in the extracellular fluid and do not cross the intact blood−brain barrier (BBB). They are often used to enhance signals of central nervous system tissues that lack a BBB (e.g., pituitary gland), extraaxial tumors (e.g., meningiomas), and areas of BBB breakdown (e.g., tumor margins). These contrast agents can also be used in a similar nontargeted manner to enhance contrast between pathologies and surrounding normal areas in other organs (4-6).

Gadolinium(III) (Gd^3+^), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective at enhancing proton relaxation because of its high magnetic moment and very labile water coordination (5, 7-9). Gadopentetate dimeglumine (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates or Gd-based contrast agents (GBCAs) have since been developed in an effort to further improve clinical efficacy, patient safety, and patient tolerance. The major chemical differences among these Gd chelates are the presence or absence of overall charge, ionic or nonionic, and their ligand frameworks (linear or macrocyclic). They are all non-targeted MRI contrast agents that are used in clinical practice.

Introduction of the lipophilic moiety, ethoxybenzyl, into the Gd chelate Gd-DTPA yielded Gd-EOB-DTPA (1). On i.v. administration, Gd-EOB-DTPA is taken up by both the liver and kidney and excreted into the urine and bile (10, 11). The uptake of Gd-EOB-DTPA by the hepatocytes allows differentiation between the healthy tissue and liver tumor because the tumorous liver tissue accumulates little Gd-EOB-DTPA (10, 12). This specific uptake mechanism is not entirely known because of evidence that the human organic anionic-transporter protein (OATP) is not involved (13). Excretion of Gd-EOB-DTPA in the bile may also permit visualization of both the gall bladder and the bile ducts. Gd-EOB-DTPA is highly soluble in water and exhibits low protein binding. Gd-EOB-DTPA is not commercially available in the United States, but it was approved as a MRI liver contrast agent in Sweden (3). In this formulation (0.25-mmol/ml injection), Gd-EOB-DTPA has an osmolality of 688 mOsm/kg H_2_0 (at 37 ºC), viscosity of 1.19 mPa.s (at 37 ºC), and pH 7.0 (14).

Both renal and extra-renal toxicities have been reported following the clinical use of gadolinium in patients with underlying kidney disease (15-17). In 2007, the US FDA (http://www.fda.gov/cder/drug/infopage/gcca/default.htm) requested manufacturers of all GBCAs to add new warnings about exposure to GBCAs increases the risk for nephrogenic systemic fibrosis (NSF) in patients with advanced kidney disease.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium%29%20AND%20synthesis)]

Schmitt-Willich et al. (2) described a detailed synthesis of Gd-EOB-DTPA by a method that started with the commercially available N_α_-benzyloxy-carbonyl-L-tyrosine methyl ester (Z-Tyr-OMe). Two different approaches to prepare the chiral triamine as a key intermediate were developed. For a small-scale synthesis, the protected amino acid Z-Tyr-OMe was O-alkylated at the phenolic function with ethyl iodide in dimethylformamide to yield O-ethyl-N_α_-benzyloxycarbonyl-L-tyrosine methyl ester. This was converted to N-(2-aminoethyl)N_α_-benzyloxycarbonyl-O-ethyl-L-tyrosinamide hydrochloride. This was then converted into N-(2-aminoethyl)-O-benzyloxycarbonyl-O-ethyl-L-tyrosinamide by aminolysis with an excess of ethylenediamine and followed by catalytic hydrogenation. This was reduced with concentrated diborane/tetrahydrofuran to S-1-(4-ethoxybenzyl)-3-azapentane-1,5-diamine trihydrochloride. For large-scale preparation, instead of aminolysis of tyrosine methyl ester, the ester was reduced to the corresponding alcohol using sodium borohydride in methanol. The obtained chiral triamine from either approach was then converted in two steps into the nonstoichiometric sodium salt (S-EOB-DTPA sodium salt). The complexation of EOB-DTPA with Gd(III) was conducted by adding gadolinium oxide (Gd_2_O_3_) to the ligand in water at 80 ºC for 1 h to produce the Gd-EOB-DTPA. The solution was filtered through a 0.2-μm filter, and the pH was adjusted to 7.0 using 1 N sodium hydroxide. The solution was added at 50ºC to ethanol. The mixture was then heated under reflux for 2 h. Precipitation from water/ethanol (85%) yielded a final product with a purity >98% determined by high-performance liquid chromatography (HPLC). Complex formation of pure S-EOB-DTPA with Gd(III) generated a second chiral center. Chiral HPLC found two diastereomers in a ratio of ~65:35.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium%29%20AND%20in%20vitro)]

Schuhmann-Giampieri et al. (1) measured the relaxivity of Gd-EOB-DTPA at 0.47 T (20 MHz) at 39 ºC. The t_1_ relaxivity values of Gd-EOB-DTPA were 5.30 ± 0.33, 8.64 ± 0.47, and 11.2 ± 0.60 liter/mmol·sec in water, plasma, and blood, respectively. It is reported that Gd-EOB-DTPA has a thermodynamic stability of log K = 23.46 (14, 18). In comparison, the value of log K for Gd-DTPA is 22.2.

Muhler et al. (11) studied the acute toxicity of Gd-EOB-DTPA (0.3 mmol/kg) in an in vitro perfused rat liver model and found no significant change in the functional parameters, enzymes, or potassium release in the liver. Pascolo et al. (13) studied the hepatic uptake mechanism of Gd-EOB-DTPA in basolateral rat hepatocyte plasma membrane vesicles (bLPMV). Gd-EOB-DTPA entered bLPMV via a linear, concentration-dependent mechanism through up to 1.5 mM of substrate. Using Xenopus laevis oocytes injected with cRNA that encoded for the human OATP and measuring the OATP transport of Gd-EOB-DTPA, the author suggested that OATP was not involved in the transport of Gd-EOB-DTPA. van Montfoort et al. (19) demonstrated saturable uptake of Gd-EOB-DTPA by the first member (Oatp1) of the polyspecific organic anion transporting polypeptides (Oatps) isolated from the rat liver. The study indicated that Gd-EOB-DTPA was a low-affinity substrate of the rat liver Oatp1.

Lewin et al. (20) evaluated the suitability of Gd-EOB-DTPA as a nonviral vector for gene therapy of hepatocellular carcinoma. Cells suspensions (10^7^ cells) of cultured rat hepatocytes and the hepatoma cells HepG2 and Huh7 were incubated with 25 μmol Gd-EOB-DTPA at 37 ºC for 15−90 min. Gd-EOB-DTPA was specifically taken up by normal rat hepatocytes but not by hepatoma cells. Incubating the cells with plasmids that contain the lacZ reporter gene and polyethyleneimine-Gd-EOB-DTPA resulted in a few transfected cells. The study suggested that the Gd-EOB-DTPA polycation conjugates could serve as transfer vectors of interest for gene-targeting imagery at the early stage of hepatocarcinogenesis. However, the transfer efficiency of the studied conjugate was low and required improvement.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium%29%20AND%20rodentia)]

Muhler and Weinmann (18) used radioactive ^153^Gd-EOB-DTPA to study the biodistribution and excretion of Gd-EOB-DTPA after repeated i.v. administration to rats. A dose of 50 μmol/kg of ^153^Gd-EOB-DTPA (a specific activity of 12.3 MBq/mmol(0.33 mCi)/mmol) was administered daily to each rat for 5 days. The injected dose was rapidly cleared from the body. Radioactivity primarily accumulated in the liver and kidneys. Approximately 81.9-82.7% of the injected dose (ID) was excreted in the feces and 17.5−18.2%ID was excreted in the urine within the first 3 days after the last dose. After 21 days, radioactivity was detected only in the kidneys, bone, stomach, and testes. The values (n = 5) were 0.409 ± 0.177, 0.239 ± 0.052, 0.037 ± 0.008 , and 0.033 ± 0.007%ID, respectively. Approximately 0.002 ± 0.177% ID was detected in the whole body. Using ^153^Gd-EOB-DTPA, Schumann-Giampieri et al. (10, 21) found non-linear pharmacokinetics for Gd-EOB-DTPA after a single i.v. bolus dose of 0.05-0.5 mmol/kg in rats. The total plasma clearance (CL) was 44.5 ± 4.87 (0.05 mmol/kg) to 24.8 ± 2.84 (0.5 mmol/kg) ml/min.kg (n = 10). Plasma binding was 10.3 ± 1.4%. V_max_ was 4.34 ± 0.58 μmol/min.kg for the 0.5-mmol/kg dose.

Schuhmann-Glampieri et al. (1) found that the acute i.v. tolerance (LD_50_) of Gd-EOB-DTPA was 10 mmol/kg in mice and rats. In rat subacute toxicity studies, all rats survived after i.v. doses of 2.5 mmol/kg four times/week for 4 weeks. Vacuolization was observed in the proximal tubuli of the kidneys, an osmotic nephrosis phenomenon that was observed with many other ionic and nonionic contrast agents. The biodistribution studies (0.25 mmol/kg Gd-EOB-DTPA) showed that the renal elimination (n = 5) was 30.5 ± 4.72% ID, and the extrarenal elimination was 62.7 ± 10.9% ID on day 7 after administration. Biliary excretion at 3 h after i.v. administration of 0.05, 0.1, 0.2, 0.5, and 1.5 mmol/kg was 80.3 ± 3.92, 68.9 ± 4.28, 63.4 ± 3.83, 53.1 ± 3.15, and 32.5 ± 5.6%, respectively. This excretion was inhibited by coadministration of sulfobromophthalein ( transported by the organic anion transporter polypeptide system into the hepatocyte). In the rat MRI (2 T) imaging study, the liver signal intensity increased 100% after 10 min. The implanted Novikoff hepatoma was clearly delineated from the normal liver tissue. In a biliary excretion and pharmacokinetics study, Schuhmann-Giampieri et al. (22) showed that the total amount of Gd-EOB-DTPA that underwent biliary excretion 0−90 min after injection was 39.5 ± 11.8% ID. The maximum excretion rate was 9.2 μmol/min per kg for the iinfustion rate of 50 μmol/min per kg. The amount of Gd-EOB-DTPA recovered in bile after the intraduodenal application of 0.1 mmol/kg was 4.61 ± 1.05% ID.

In a comparison study, Van Beers et al. (23) compared the enhancement pattern of rat hepatocellular carcinomas (HCCs) by Gd-EOB-DTPA (0.06 mmol/kg) with ^99m^Tc-iminodiacetic acid (^99m^Tc-IDA; 3−22.2 MBq (0.08-0.6 mCi)). With Gd-EOB-DTPA t_1_-weighted spin-echo MRI (200 MHz), the peak liver enhancement (relative intensity (RI_post_) − RI_pre_ /RI_pre_ × 100) was 127% at 5 min and the peak tumor enhancement was 66% at 5 min. In comparison, the mean ^99m^Tc-IDA radioactivity uptake was 215% ID/100 g in the liver and 95% ID/100 g in the tumor at 5 min after administration. The study concluded that the enhancement pattern of HCCs with Gd-EOB-DTPA was different from that of ^99m^Tc-IDA.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

In a pharmacokinetics study, Schuhmann-Giampieri, et al. (10, 21) injected bolus doses of 0.03 and 0.25 mm/kg ^153^Gd-EOB-DTPA into 5 female beagle dogs and found nonlinear pharmacokinetics. The CL was 18.2 ± 3.27 (at the 0.03 mmol/kg dose) to 12.2 ml/min per kg (0.25 mmol/kg), and the renal CL (CL_R_) was 3.74 ± 1.00 (0.03-mmol/kg) to 3.88 ± 0.71 ml/min per kg (0.25 mmol/kg). V_max_ was 2.40 ± 0.98 μmol/min per kg at the 0.25 mmol/kg dose. After 7 days, the urinary excretion was 27.1 ± 2.08 (0.03 mmol/kg) to 40.9 ± 2.35%ID (0.25 mmol/kg). The % ID fecal excretion was 70.1 ± 3.25 to 57.0 ± 2.48 for the low dose and high doses, respectively.

Benness et al. (24, 25) studied the hepatic kinetics and MRI (1.5 T) of Gd-EOB-DTPA in dogs. After bolus injection, there was a rapid increase and exponential decline of plasma Gd-EOB-DTPA concentration. Rapid accumulation of Gd-EOB-DTPA in the liver was demonstrated by very early positive enhancement. The study showed that a hepatic transport maximum of 0.09−0.15 μmol/min per kg was achieved with bolus doses (12.5−200 μmol/kg) followed by infusion (0.4−6.4 μmol/kg). Maximum t_1_ signal enhancement was achieved with blood concentration of 0.02−0.03 μmol/ml and a liver concentration of 1−2 μmol/ml.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium%29%20AND%20%28primate%20NOT%20human%29)]

Schuhmann-Glampieri et al. (1) studied the elimination and biodistribution of Gd-EOB-DTPA (0.25-mmol/kg) in two female cynomolgus monkeys. Seven days after administration, the percent injected dose values in the major organs were 0.28−0.52 (liver), 0.03−0.14 (kidneys), 0.04−0.12 (spleen), and 0.16−0.61 (GI tract). Approximately 47.8−63.2% ID was excreted in the urine, and 32.2-34.0% ID was excreted in the feces. In another study, Shuhmann-Giampieri et al. (10, 21) reported a CL of 2.93 ± 1.06 ml/min per kg and a CL_R_ of 1.01 ± 0.26 ml/min per kg after a single i.v. dose of 0.25 mmol/kg in 5 female cynomolgus monkeys. Vmax was 0.81 ± 0.66 μmol/min.kg for the 0.25-mmol/kg dose.. After 7 days, the renal, fecal, and total body recovery values were 44.0 ± 14.1, 32.1 ± 6.41, and 76.0 ± 11.6% ID, respectively. Plasma binding was 17.5 ± 1.0%.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gd-EOB-DTPA%20OR%20Gadoxetic%20Acid%20OR%20Eovist%20OR%20Primovist%20OR%20gadoxate%20disodium%29%20AND%20Human)]

Schuhmann-Giampieri et al. (26) studied the pharmacokinetics of Gd-EOB-DTPA in 23 healthy young male volunteers. Single doses of 0.2, 0.35, and 0.5 mmol/kg (in 0.25 mol/liter) were administered as a 10-min infusion into each volunteer. Serum concentrations declined rapidly and then the decline slowed and appeared to be log-linear. The major pharmacokinetic parameters (ranges for 0.2 mmol/kg to 0.5 mmol/kg) were calculated to be 1.86 ± 0.20 to 3.12 ± 0.78 h (serum t_½_), 2.01 ± 0.18 to 2.21 ± 0.31 h (urine t_½_), 0.55 ± 0.03 to 0.38 ± 0.05 liter/kg (Vd_ss_), 2.72 ± 0.18 to 2.13 ± 0.16 ml/min per kg (total serum CL), and 1.18 ± 0.23 to 1.25 ± 0.11 ml/min per kg (CL_R_). The 6-day cumulative renal excretion was 43.6 ± 8.6 to 59.1 ± 5.6% ID. The 6-day cumulative extrarenal excretion in the feces was 36.8 ± 8.5 to 27.1 ± 8.1% ID. The urinary excretion was rapid and independent of the dose, CL_R_ was ~100 ml/min which indicated that glomerular filtration was the main pathway of renal elimination. Gd-EOB-DTPA was generally well tolerated with no serious adverse events.

In a phase I clinical evaluation of Gd-EOB-DTPA as a hepatobiliary MRI agent, Hamm et al. (27) studied 60 healthy male volunteers. The doses ranged from 10 to 100 μmol/kg. In the tolerance and safety studies of 44 volunteers, Gd-EOB-DTPA was generally well tolerated. The biexponential decay of serum Gd concentrations could be described with a two-compartment model. Practically independent of dose, the compound was completely eliminated in urine and feces in nearly equal amounts. Reverse-phase HPLC analysis of urine samples 2 hours after injection showed no conversion of Gd-EOB-DTPA to a new compound. MRI imaging (1.5 T) of 16 volunteers showed homogeneous enhancement of liver parenchyma immediately after injection. Peak liver signal intensity was observed at 20 min after injection. This was followed by plateau-like enhancement over 2 h. Bollow et al. (28) reported that the common bile duct showed intense signal enhancement that began 5-16 min after injection and persisted for 120−360 min. Gallbladder contrasting was achieved in all 16 volunteers. The dosage for hyperintense visualization of intrahepatic duct was 10 μmol/kg.

Reimer et al. (29) reported the results of a phase II clinical evaluation of Gd-EOB-DTPA. A randomized double-blind trial was performed in 33 patients with focal solid liver lesions. Three different doses (12.5, 25, and 50 μmol/kg) were studied with MRI (1.0 T). All doses increased liver signal intensity and lesion-liver C/N ratios ([mean signal intensity of lesion –mean signal intensity of liver]/standard deviation of background noise). The lowest dose (12.5 μmol/kg) was sufficient to enhance the detection of focal liver lesions. Depending on the imaging techniques, the lesion-liver C/N ratios (n = 10) for liver metastases ranged from 6.4 ± 3.9 to 16.0 ± 9.2 (eight techniques) at 20 min after injection. At 45 min, the C/N ratios were 10.7 ± 4.0 to 14.9 ± 9.2 (four techniques). No significant changes in vital signs, clinical laboratory test results, or urinalysis were observed. In the multicenter phase III efficacy and safety clinical trial, Bluemke, et al. (30) studied 172 patients with liver lesions from 12 medical centers. All patients received 25 μmol/kg of Gd-EOB-DTPA as an i.v. bolus injection (2 ml/sec). MRI was performed by 1.5-T systems to obtain both t_1_-weighted and t_2_-weighted images. For the total number of lesions that were correctly detected and classified as benign or malignant by three blinded readers, the ranges of sensitivity for precontrast MRI (t_1_-weighted and t_2_-weighted, t_1_-weighted), postcontrast MRI (t_1_-weighted and t_2_-weighted, t_1_-weighted), combined pre- and postcontrast MRI, and helical CT were 49.1−63.8, 59.0−72.8, 65.9−70.0, and 60.0−68.4%, respectively. Overall, there were 28 adverse events in 17 (10.0%) of 169 patients. Only one event was classified as definitely related to the contrast agent. All events were mild or moderate in intensity.

## References

1 Schuhmann-Giampieri G., Schmitt-Willich H., Press W.R., Negishi C., Weinmann H.J., Speck U. (1992). Preclinical evaluation of Gd-EOB-DTPA as a contrast agent in MR imaging of the hepatobiliary system. Radiology.
2 Schmitt-Willich H., Brehm M., Ewers C.L., Michl G., Muller-Fahrnow A., Petrov O., Platzek J., Raduchel B., Sulzle D. (1999). Synthesis and Physicochemical Characterization of a New Gadolinium Chelate: The Liver-Specific Magnetic Resonance Imaging Contrast Agent Gd-EOB-DTPA. Inorg Chem.
3 (2004). Gadoxate disodium: gadolinium EOB DTPA, gadoxetic acid, Gd-EOB-DTPA. Drugs R D.
4. Brasch, R.C., M.D. Ogan and B.L. Engelstad, Paramagnetic Contrast Agents and Their Application in NMR Imaging, in Contrast media; Biologic effects and clinical application, Z. Parvez, R., R. Monada and M. Sovak, Editor. 1987, CRC Press, Inc.: Boca Raton, Florida. p. 131-143.
5. Saini, S., J.T. Ferrucci, Enhanced Agents for Magnetic Resonance Imaging: Clinical Applications, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 662-681.
6 Runge V.M., Kirsch J.E., Wells J.W., Awh M.H., Bittner D.F., Woolfolk C.E. (1993). Enhanced liver MR: Contrast agents and imaging strategy. Critical Reviews in Diagnostic Imaging.
7 DeSimone D., Morris M., Rhoda C., Lucas T., Zielonka J., Olukotun A., Carvlin M. (1991). Evaluation of the safety and efficacy of gadoteridol injection (a low osmolal magnetic resonance contrast agent). Clinical trials report. Invest Radiol.
8 Wedeking P., Kumar K., Tweedle M.F. (1992). Dissociation of gadolinium chelates in mice: relationship to chemical characteristics. Magn Reson Imaging.
9 Yuh W.T., Engelken J.D., Muhonen M.G., Mayr N.A., Fisher D.J., Ehrhardt J.C. (1992). Experience with high-dose gadolinium MR imaging in the evaluation of brain metastases. AJNR Am J Neuroradiol.
10 Schuhmann-Giampieri G. (1993). Nonlinear pharmacokinetic modeling of a gadolinium chelate used as a liver-specific contrast agent for magnetic resonance imaging. Arzneimittelforschung.
11 Muhler A., Clement O., Saeed M., Lake J.R., Stites D.P., Berthezene Y., Brasch R.C. (1993). Gadolinium-ethoxybenzyl-DTPA, a new liver-directed magnetic resonance contrast agent. Absence of acute hepatotoxic, cardiovascular, or immunogenic effects. Invest Radiol.
12 Reimer P., Schneider G., Schima W. (2004). Hepatobiliary contrast agents for contrast-enhanced MRI of the liver: properties, clinical development and applications. Eur Radiol.
13 Pascolo L., Cupelli F., Anelli P.L., Lorusso V., Visigalli M., Uggeri F., Tiribelli C. (1999). Molecular mechanisms for the hepatic uptake of magnetic resonance imaging contrast agents. Biochem Biophys Res Commun.
14 (2002). Primovist, detailed product information, Schering AG. p. 1-8.
15 Perazella M.A., Rodby R.A. (2007). Gadolinium use in patients with kidney disease: a cause for concern. Semin Dial.
16 Grobner T., Prischl F.C. (2007). and Gadolinium and nephrogenic systemic fibrosis. Kidney Int.
17 Pedersen M. (2007). Safety update on the possible causal relationship between gadolinium-containing MRI agents and nephrogenic systemic fibrosis. J Magn Reson Imaging.
18 Muhler A., Weinmann H.J. (1995). Biodistribution and excretion of 153Gd-labeled gadolinium ethoxybenzyl diethylenetriamine pentaacetic acid following repeated intravenous administration to rats. Acad Radiol.
19 van Montfoort J.E., Stieger B., Meijer D.K., Weinmann H.J., Meier P.J., Fattinger K.E. (1999). Hepatic uptake of the magnetic resonance imaging contrast agent gadoxetate by the organic anion transporting polypeptide Oatp1. J Pharmacol Exp Ther.
20 Lewin M., Clement O., Belguise-Valladier P., Tran L., Cuenod C.A., Siauve N., Frija G. (2001). Hepatocyte targeting with Gd-EOB-DTPA: potential application for gene therapy. Invest Radiol.
21 Schuhmann-Giampieri G., Frenzel T., Schmitt-Willich H. (1993). Pharmacokinetics in rats, dogs and monkeys of a gadolinium chelate used as a liver-specific contrast agent for magnetic resonance imaging. Arzneimittelforschung.
22 Schuhmann-Giampieri G., Schmitt-Willich H., Frenzel T., Schitt-Willich H. (1993). Biliary excretion and pharmacokinetics of a gadolinium chelate used as a liver-specific contrast agent for magnetic resonance imaging in the rat. J Pharm Sci.
23 Van Beers B.E., Grandin C., Pauwels S., Mottet I., Goudemant J.F., Delos M., Demeure R., Pringot J. (1994). Gd-EOB-DTPA enhancement pattern of hepatocellular carcinomas in rats: comparison with Tc-99m-IDA uptake. J Magn Reson Imaging.
24 Benness G., Khangure M., Morris I., Warwick A., Burrows P., Vogler H., Weinmann H.J. (1996). Hepatic kinetics and magnetic resonance imaging of gadolinium-EOB-DTPA in dogs. Invest Radiol.
25 Benness G., Khangure M., Morris I., Warwick A., Burrows P., Vogler H. (1994). Kinetics and magnetic resonance imaging of Gd-EOB-DTPA in dogs. Invest Radiol.
26 Schuhmann-Giampieri G., Mahler M., Roll G., Maibauer R., Schmitz S. (1997). Pharmacokinetics of the liver-specific contrast agent Gd-EOB-DTPA in relation to contrast-enhanced liver imaging in humans. J Clin Pharmacol.
27 Hamm B., Staks T., Muhler A., Bollow M., Taupitz M., Frenzel T., Wolf K.J., Weinmann H.J., Lange L. (1995). Phase I clinical evaluation of Gd-EOB-DTPA as a hepatobiliary MR contrast agent: safety, pharmacokinetics, and MR imaging. Radiology.
28 Bollow M., Taupitz M., Hamm B., Staks T., Wolf K.J., Weinmann H.J. (1997). Gadolinium-ethoxybenzyl-DTPA as a hepatobiliary contrast agent for use in MR cholangiography: results of an in vivo phase-I clinical evaluation. Eur Radiol.
29 Reimer P., Rummeny E.J., Shamsi K., Balzer T., Daldrup H.E., Tombach B., Hesse T., Berns T., Peters P.E. (1996). Phase II clinical evaluation of Gd-EOB-DTPA: dose, safety aspects, and pulse sequence. Radiology.
30 Bluemke D.A., Sahani D., Amendola M., Balzer T., Breuer J., Brown J.J., Casalino D.D., Davis P.L., Francis I.R., Krinsky G., Lee F.T., Lu D., Paulson E.K., Schwartz L.H., Siegelman E.S., Small W.C., Weber T.M., Welber A., Shamsi K. (2005). Efficacy and safety of MR imaging with liver-specific contrast agent: U.S. multicenter phase III study. Radiology.